# ^99m^Tc-Labeled mannosylated dextran DCM20

Chemical name: | ^99m^Tc-Labeled mannosylated dextran DCM20 | [image]
Abbreviated name: | ^99m^Tc(CO)_3_-DCM20 | [image]
Synonym: | 7 | [image]
Agent Category: | Compounds | [image]
Target: | Mannose Receptors | [image]
Target Category: | Receptors | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of the probes by Pirmettis et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%20sentinel%20lymph%20node%20and%20imaging)]

^99m^Tc-Labeled mannosylated dextran DCM20, abbreviated as ^99m^Tc(CO)_3_-DCM20, is a dextran derivative bearing S-derivatized cysteine chelator and mannose moieties. ^99m^Tc(CO)_3_-DCM20 was synthesized by Pirmettis et al. for sentinel lymph node (SLN) detection (1). SLN is defined as the first node in the lymphatic basin that receives the primary lymphatic flow.

The concept of SLN is embedded with the notion that the metastatic spread of solid tumors through lymphatic vessels follows a predictable pattern, i.e., tumor cells metastasize to the first lymph node encountered by lymphatic draining from the primary tumor (the SLN), followed by the second- and third-tier lymph nodes; being able to determine the status of the SLN with or without metastatic involvement would allow accurate prediction of the status of the entire regional lymphatic basin draining the tumor (2). Based on this concept, a SLN free from tumor metastasis would exclude tumor spread to the at-risk regional lymphatic basin, rendering nodal basin dissection unnecessary and avoiding the immediate and late complications caused by nodal dissection (3).

The concept of SLN has now been widely accepted in clinical practice, and the technology for guided SLN biopsy has been evolving rapidly. Compared with other methods, γ-probe–guided SLN biopsy appears to be more cost-effective, and substantial work has been done in developing optimal imaging techniques and radiotracers to visualize the lymphatic channels leading from the site of tracer administration to the corresponding lymph nodes and to identify the SLN encountered along the lymphatic pathway (2, 3). Currently, three types of radiocolloid preparations are commonly used for lymphoscintigraphy combined with intraoperative γ-probe SLN identification. The ^99m^Tc-sulfur colloid is the most commonly used probe in the United States (2). The probes are given through peritumoral, periareolar, or dermal injection; from the injection site, the probe particles migrate into the lymphatic vessels by passive diffusion. For most probes, intranodal retention is a process of active, saturable phagocytosis of the macrophages lining the sinusoid spaces of lymph nodes (4, 5). The particle size and surface characteristics of probes influence not only the rate of colloid drainage from the injection site to the lymphatic capillaries but also the phagocytosis by lymph node macrophages. Particles <5 nm easily leak into the bloodstream, whereas particles >100 nm are often trapped in the interstitial space, resulting in masking of the SLN (1, 2, 6).

Studies have shown that introduction of mannose molecules to ^99m^Tc-labeled macromolecules like albumin, polylysine, and dextrans enhances the retention of these probes in the SLN in a saturable mode because of the recognition by the mannose receptors of lymph node macrophages, even though the particles are only a few nanometers in size (7, 8). Pirmettis et al. synthesized a mannosylated nanocompound DCM20, which has a dextran backbone, S-derivatized cysteines as a chelator for labeling with the [^99m^Tc(CO)_3_]^+^ core, and mannose moieties for binding with mannose receptors (1). The radiolabeled DCM20 (^99m^Tc(CO)_3_-DCM20) exhibited fast injection site clearance and high uptake and retention in the SLN. This chapter summarizes the data obtained with ^99m^Tc(CO)_3_-DCM20.

### Related Resource Links:

Protein sequences of mannose receptor (http://www.ncbi.nlm.nih.gov/protein?term=mannose%20receptor)

Mannose compound information (http://www.ncbi.nlm.nih.gov/pcsubstance?term=mannose%20receptor) in PubChem

Mannose receptor-related articles (http://www.ncbi.nlm.nih.gov/omim?term=mannose%20receptor) in Online Mendelian Inheritance in Man

Mannose receptor-targeted probes (http://www.ncbi.nlm.nih.gov/books/?term=mannose+receptor+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22519912)]

Pirmettis et al. prepared DCM20 in three steps, with all products being purified with ultrafiltration and their identity being established with full ^1^H and ^13^C nuclear magnetic resonance assignments (1). First, the reaction of dextran (MW 11,800 g/mol, glucopyranose units = 73) with excess allyl bromide yielded the intermediate allyl dextran (MW 13,030 g/mol, allyl = 30, yield = 86%). Second, addition of L-cysteine converted allyl dextran to DC15 through thiol-ene "click" reaction, which resulted in the incorporation of S-derivatived cysteines in the dextran molecules (yield = 78%). DC15 was then reacted with freshly prepared 2-imino-2-methoxyethyl-1-thio-β-D-mannoside solution to generate the mannosylated dextran DCM20 in which mannose groups were introduced through formation of an amidino linkage with the amino groups of S-derivatized cysteines. The extent of cysteine mannosylation was ~81%. The sugar contents of DC15 and DCM20 were estimated to be 73 ± 2 and 94 ± 3 sugar units, respectively.

DC15 and DCM20 were labeled with ^99m^Tc by the [^99m^Tc(CO)_3_]^+^ precursor at ligand concentrations of 10−^5^−10−^6^ M, which led to the generation of ^99m^Tc(CO)_3_-DC15 and ^99m^Tc(CO)_3_-DCM20, respectively (1). High-performance liquid chromatography (HPLC) showed the absence of any ^99m^TcO_4_− (t_R_ = 3.5 min) and quantitative conversion (>95%) of the precursor (t_R_ = 4.5 min) to a single ^99m^Tc(CO)_3_-DC15 (t_R_ = 11.9) or ^99m^Tc(CO)_3_-DCM20 (t_R_ = 12.5 min) in high radiochemical yields (95%), even at low ligand concentration (1.5 × 10−^6^ M). Pirmettis et al. also performed the labeling in one pot by mixing and boiling 50 μg freeze-dried DCM20 with 1.5 mL pertechnetate into the Isolink vial for 30 min, which demonstrated the feasibility of developing a single-vial kit containing all the required ingredients for labeling.

Periodic HPLC analysis of ^99m^Tc(CO)_3_-DC15 and ^99m^Tc(CO)_3_-DCM20 for up to 24 h did not show any significant changes in the chromatograms, even after 1:20 dilution in saline and phosphate-buffered saline (PBS), suggesting that the ^99m^Tc-complexes were stable. The in vitro stability of ^99m^Tc(CO)_3_-DC15 and ^99m^Tc(CO)_3_-DCM20 toward transchelation was evaluated by incubating for 1–6 h at 37ºC with a large excess (20-fold) of the amino acids cysteine or histidine. Both cysteine and histidine have high affinity for the fac-[^99m^Tc(CO)_3_]^+^ synthon. In both cases, the ^99m^Tc-complexes presented high radiochemical purity (≥90%), suggesting they had no transchelation with either cysteine or histidine.

To investigate the coordination of DCM20 with the fac-[^99m^Tc(CO)_3_]^+^ core, Pirmettis et al. prepared macroscopic amounts of the rhenium complexes of both DC15 and DCM20 (1). Rhenium is the group VIIB congener of technetium and is often used as a nonradioactive alternative to technetium for large-scale synthesis and structural characterization. Reaction of DC15 or DCM20 with the [NEt_4_]_2_[ReBr_3_(CO)_3_] precursor led to the formation of complexes Re(CO)_3_-DC15 (yield = 76%) and Re(CO)_3_-DCM20 (yield = 81%), respectively. Dynamic light-scattering studies showed that the hydrodynamic diameters of the particles increased slightly with the modifications introduced on the dextran backbone (Table 1). Addition of 30 propylene-S-cysteine groups, 24 of them being mannosylated, resulted in DCM20 with a diameter of 6.5 ± 0.5 nm. Coordination with the rhenium tricarbonyl unit increased the hydrodynamic diameter of Re(CO)_3_-DCM20 to 8.3 ± 0.5 nm, suggesting that the analogous ^99m^Tc(CO)_3_-DCM20 may display a hydrodynamic diameter in the range of 6.5−8.3 nm. Zeta potential measurements revealed a negative charge for DCM20 (−6.3 ± 0.1 mV). Complexation of DCM20 with the Re(CO)_3_^+^ core did not affect the charge of the final compound Re(CO)_3_-DCM20 (−6.3 ± 0.1 mV). Based on the intensity of the αCH peak of the re-coordinated cysteine in the NMR spectra, it was estimated that on average 2−3 fac-[Re(CO)_3_]^+^ cores were coordinated per molecule of dextran.

Table 1: Characteristics of the probes

Compound | Cysteine | Mannose | Diameter (nm) | Zeta potential (mV) | MW (g/mol)
DCM20 | 6 | 24 | 6.5 ± 0.5 | –6.3 ± 0.1 | 22,270
DC15 | 30 | none | nd | nd | 16,630
Re(CO)_3_-DCM20 | 6 | 24 | 8.3 ± 0.5 | –6.3 ± 0.1 | 23,083
Re(CO)_3_-DC15 | 30 | none | nd | nd | 20,680

*MW, calculated; nd, not determined.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22519912)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22519912)]

The biological evaluation of ^99m^Tc(CO)_3_-DCM20 was performed with biodistribution studies and single-photon emission computed tomography/computed tomography (SPECT/CT) in mice after subcutaneous injection into mouse footpad (1). For comparison purposes, the non-mannosylated analogs ^99m^Tc(CO)_3_-DC15 and ^99m^Tc-phytate were also tested under the same conditions. ^99m^Tc-Phytate is a radiopharmaceutical approved in Japan for SLN detection. For biodistribution studies, 2 × 10^–12^ mol/20 µl of each probe was injected and animals were euthanized at different time points after injection (n = 3 mice/group per time point). For SPECT/CT imaging, 2 × 10^–11^ mol/20 µl of each probe was given to mice.

For ^99m^Tc(CO)_3_-DCM20, the uptake in the popliteal lymph node (the SLN in this case) was 9.2, 7.8, and 7.0% injected dose (ID) at 0.5, 1, and 6 h after injection, respectively. The radioactivity levels at the injection site dropped to 67% ID at 30 min and to 55% ID at 1 h, and then remained stable for up to 6 h after injection. For ^99m^Tc-phytate, the uptake was 3% ID in popliteal lymph node and 80% ID at the injection site at all time points studied. The radioactivity levels in the blood and liver were very low for both ^99m^Tc(CO)_3_-DCM20 and ^99m^Tc-phytate. For ^99m^Tc(CO)_3_-DC15, it showed fast clearance from the injection site; however, only marginal uptake in the popliteal lymph node was observed, accompanied by high radioactivity levels in the blood.

SPECT/CT imaging showed that the popliteal lymph node was clearly delineated at 30 min after injection of ^99m^Tc(CO)_3_-DCM20, with an injection site/SLN radioactivity ratio of 4.7 (n = 2 mice). The second and third lymph nodes, accumulating smaller amounts of radioactivity, could also be visualized with injection site/SLN ratios of 15.2 and 49.3, respectively. For ^99m^Tc-phytate, the popliteal lymph node was delineated at 6 h after injection, while most of the radioactivity remained at the injection site, resulting in an injection site/SLN ratio of 70.4 (n = 2 mice). Imaging with ^99m^Tc(CO)_3_-DC15 showed faint radioactivity in the popliteal lymph node, with ~50% of the radioactivity being cleared from the injection site and accumulating in the urinary bladder at 30 min after injection, resulting in an injection site/SLN ratio of 47.3 (n = 2 mice). These findings indicate that ^99m^Tc(CO)_3_-DCM20 is promising and merits further evaluation as a radiopharmaceutical probe for SLN detection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22519912)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22519912)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22519912)]

No references are currently available.

## References

1 Pirmettis I., Arano Y., Tsotakos T., Okada K., Yamaguchi A., Uehara T., Morais M., Correia J.D., Santos I., Martins M., Pereira S., Triantis C., Kyprianidou P., Pelecanou M., Papadopoulos M. (2012). New (99m)Tc(CO)(3) Mannosylated Dextran Bearing S-Derivatized Cysteine Chelator for Sentinel Lymph Node Detection. Mol Pharm.
2 Mariani G., Erba P., Villa G., Gipponi M., Manca G., Boni G., Buffoni F., Castagnola F., Paganelli G., Strauss H.W. (2004). Lymphoscintigraphic and intraoperative detection of the sentinel lymph node in breast cancer patients: the nuclear medicine perspective. J Surg Oncol.
3 Noguchi M. (2002). Sentinel lymph node biopsy and breast cancer. Br J Surg.
4 Rubello D., Zavagno G., Bozza F., Lise M., De Salvo G.L., Saladini G., Mariani G., Casara D. (2004). Analysis of technical and clinical variables affecting sentinel node localization in patients with breast cancer after a single intradermal injection of 99mTc nanocolloidal albumin. Nucl Med Commun.
5 Wallace A.M., Hoh C.K., Darrah D.D., Schulteis G., Vera D.R. (2007). Sentinel lymph node mapping of breast cancer via intradermal administration of Lymphoseek. Nucl Med Biol.
6 Jeong J.M., Hong M.K., Kim Y.J., Lee J., Kang J.H., Lee D.S., Chung J.K., Lee M.C. (2004). Development of 99mTc-neomannosyl human serum albumin (99mTc-MSA) as a novel receptor binding agent for sentinel lymph node imaging. Nucl Med Commun.
7 Karagiorgou O., Patsis G., Pelecanou M., Raptopoulou C.P., Terzis A., Siatra-Papastaikoudi T., Alberto R., Pirmettis I., Papadopoulos M. (2005). (S)-(2-(2'-Pyridyl)ethyl)cysteamine and (S)-(2-(2'-pyridyl)ethyl)-d,l-homocysteine as ligands for the "fac-[M(CO)(3)](+)" (M = Re, (99m)Tc) core. Inorg Chem.
8 Takagi K., Uehara T., Kaneko E., Nakayama M., Koizumi M., Endo K., Arano Y. (2004). ^ 99m ^ Tc-labeled mannosyl-neoglycoalbumin for sentinel lymph node identification. Nucl Med Biol.